# ^111^In-(1-isothiocyanatobenzyl-3-methyldiethylenetriaminepentaaetic acid)-anti–TAG-72 humanized C_H_2 domain-deleted antibody

Chemical name: | ^111^In-(1-isothiocyanatobenzyl-3-methyldiethylenetriaminepentaacetic acid)-anti–TAG-72 humanized C_H_2 domain-deleted antibody
Abbreviated name: | ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab
Synonym: | ^111^In-HuCC49ΔC_H_2 Ab, ^111^In-CC49 Ab
Agent Category: | Humanized C_H_2 domain-deleted antibody variant
Target: | (Sialyl-Tn) TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal /contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2)]

^111^In-(1-isothiocyanatobenzyl-3-methyldiethylenetriaminepentaacetic acid)-anti–TAG-72 humanized C_H_2 domain-deleted antibody (^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab), which is formed by the conjugation of ^111^In with a bioengineered anti–tumor-associated glycoprotein 72 (TAG-72) antibody construct, has been developed for single-photon emission computed tomography (SPECT) imaging of cancers that express TAG-72 (1). ^111^In is a gamma emitter with a half-life (t_½_) of 2.8 d.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (2-5). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (6). The murine monoclonal antibody B72.3 (MAb B72.3) against TAG-72 was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (7). With use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-2 monoclonal antibodies with higher affinity constants (K_a_) have been produced and characterized (2, 3, 7, 8). CC49 MAb appears to react with a unique disaccharide Sialyl-Tn (STn) epitope on the TAG-72 (9).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (10). Radiolabeled B72.3 and CC49 have shown excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (11, 12). Because of their relatively large sizes, radiolabeled intact MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (8, 13-15). One approach to minimize these problems is breaking up intact antibodies into antibody fragments such as F(ab’)_2_ and Fab’ (16). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (8, 17, 18). The removal of the C_H_2 domain of IgG also appears to result in a significantly faster blood clearance and more rapid tumor uptake (1, 19, 20). Slavin-Chiorini et al. (21) bioengineered a complementary determining region-grafted humanized CC49 MAb (HuCC49) with a C_H_2 domain deletion (ΔC_H_2). Radiolabeled HuCC49ΔC_H_2 constructs have demonstrated faster blood clearance in mice (1, 21, 22). Clinical studies with radioiodinated HuCC49ΔC_H_2 Ab in patients did show faster blood clearance (23). Chinn et al. (1) prepared and evaluated ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab as a potential SPECT imaging molecular probe for tumors expressing TAG-72.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2+)]

Chinn et al. (1) reported the preparation and radiolabeling of HuCC49ΔC_H_2 . Kashmiri et al. (24) prepared the humanized CC49 MAb by grafting the CC49 MAb hypervariable regions onto the variable light and variable heavy frameworks of the human MAbs LEN and 21/28’ CL, respectively. Slavin-Chiorini et al. (21) described the development of the HuCC49ΔC_H_2 Ab from the humanized CC49 MAb. Before conjugation to Mx-DTPA, the HuCC49ΔC_H_2 Ab was diafiltrated at 2–8º into metal-free 0.9% sodium chloride. The pH of the solution was adjusted to 8.6 in sodium borate–buffered saline. This HuCC49ΔC_H_2 Ab solution was reacted with Mx-DTPA in a chelator/protein molar ratio of 3:1. The reaction mixture was incubated overnight for 16–20 h at ambient temperature. The unreacted Mx-DTPA was removed by diafiltration. This resulted in 1.1 mol Mx-DTPA per mol of HuCC49ΔC_H_2 Ab. Radiolabeling was conducted by using ^111^In chloride (^111^InCl_3_) solution in a specific activity of 74–148 MBq/mg (2–4 mCi/mg) or 8.97–17.76 MBq/nmol (0.24–0.49 mCi/nmol) based on a molecular weight of 121 kDa. The ^111^InCl_3_ solution was first adjusted to pH 6 with sodium citrate. (Mx-DTPA)-HuCC49ΔC_H_2 was added to the ^111^InCl_3_ solution and incubated for 15 min at ambient temperature. The reaction was quenched by adding human serum albumin and diethylenetriaminepentaacetic acid (DTPA). The radiochemical yield and radiochemical purity of ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab was 97.1%. The final specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2+)]

Chinn et al. (1) conducted in vitro solid-phase competition immunoassays of (Mx-DTPA)-HuCC49ΔC_H_2 with bovine submaxillary mucin (BSM) as the TAG-72 antigen source and Eu-labeled HuCC49ΔC_H_2 Ab as a tracer. The 50% inhibitory concentration value (IC_50_) and apparent affinity constant (K_a_) of unlabeled (Mx-DTPA)-HuCC49ΔC_H_2 Ab were 15 nM and 4.20 nM, respectively. In comparison, the IC_50_ and K_a_ of Mx-DTPA-chimeric CC49 Ab (cCC49 Ab) were 5.8 nM and 0.62 nM, respectively. For ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab, immunoreactivity assays were performed with BSM-coated resin. The immunoreactivity of HuCC49ΔC_H_2 Ab was 83.8%. In comparison, the immunoreactivity of ^111^In-(Mx-DTPA)-cCC49 was 80.5% of binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2+)]

Pharmacokinetics studies of ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab were performed in normal nude mice (1). Each mouse received 74 kBq/1.3 μg (2 μCi/1.3 μg) of ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab by i.v. administration. The blood clearance appeared to be monoexponential, and the biological t_½_ in the blood was 5.4 h. The radioactivity levels (n = 3–5) in percentage injected dose per gram (% ID/g) in the blood were 43.3 at 1 h and then fell to <1 at 24 h. Tumor localization of ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab was evaluated in nude mice bearing LS-174T s.c. tumors expressing TAG-72 (~10 mm diameter) (1). Each mouse received 0.37 MBq (10 μCi) ^111^In-(Mx-DTPA)-HuCC49ΔC_H_2 Ab. The tumor radioactivity levels (n = 3) were 7.9 ± 0.7% ID/g and 14.4 ± 2.3 at 1 h and 24 h, respectively. The blood radioactivity levels were 25.5 ± 0.4% ID/g and 0.9 ± 0.1% ID/g at 1 h and 24 h, respectively. The tumor/blood ratios were 0.31 and 16.0 at 1 h and 24 h, respectively. In comparison, the tumor/blood ratios for ^111^In-Mx-DTPA-cCC49 were 0.35 and 3.7, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2+AND+human)]

No publication is currently available.

## NIH Support

NIH Intramural Support.

## References

1 Chinn P.C., Morena R.A., Santoro D.A., Kazules T., Kashmiri S.V., Schlom J., Hanna N., Braslawsky G. (2006). Pharmacokinetics and tumor localization of (111)in-labeled HuCC49DeltaC(H)2 in BALB/c mice and athymic murine colon carcinoma xenograft. Cancer Biother Radiopharm.
2 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
3 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
4 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
5 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
6 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
7 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
8 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
9 Colcher D., Pavlinkova G., Beresford G., Booth B.J., Batra S.K. (1999). Single-chain antibodies in pancreatic cancer. Ann N Y Acad Sci.
10 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
11 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
12 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
13 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
14 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
15 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
16 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
17 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
18 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
19 Mueller B.M., Reisfeld R.A., Gillies S.D. (1990). Serum half-life and tumor localization of a chimeric antibody deleted of the CH2 domain and directed against the disialoganglioside GD2. Proc Natl Acad Sci U S A.
20 Slavin-Chiorini D.C., Horan Hand P.H., Kashmiri S.V., Calvo B., Zaremba S., Schlom J. (1993). Biologic properties of a CH2 domain-deleted recombinant immunoglobulin. Int J Cancer.
21 Slavin-Chiorini D.C., Kashmiri S.V., Lee H.S., Milenic D.E., Poole D.J., Bernon E., Schlom J., Hand P.H. (1997). A CDR-grafted (humanized) domain-deleted antitumor antibody. Cancer Biother Radiopharm.
22 Slavin-Chiorini D.C. Kashmiri S.V. Schlom J. Calvo B. Shu L.M. Schott M.E. Milenic D.E. Snoy P. Carrasquillo J. Anderson K. Biological properties of chimeric domain-deleted anticarcinoma immunoglobulins Cancer Res 1995 55Suppl23 5957s 5967s 7493377
23 Forero A., Meredith R.F., Khazaeli M.B., Carpenter D.M., Shen S., Thornton J., Schlom J., LoBuglio A.F. (2003). A novel monoclonal antibody design for radioimmunotherapy. Cancer Biother Radiopharm.
24 Kashmiri S.V., Shu L., Padlan E.A., Milenic D.E., Schlom J., Hand P.H. (1995). Generation, characterization, and in vivo studies of humanized anticarcinoma antibody CC49. Hybridoma.